# ^67^Ga-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-Gly-Glu-c[Lys-Nlc-Glu-His-D-Phe-Arg-Trp-Gly-Arg-Pro-Val-Asp]

Chemical name: | ^67^Ga-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-Gly-Glu-c[Lys-Nlc-Glu-His-D-Phe-Arg-Trp-Gly-Arg-Pro-Val-Asp]
Abbreviated name: | ^67^Ga-DOTA-GlyGlu-CycMSH
Synonym:
Agent category: | Peptide
Target: | Melanocortin-1 receptor, MC1R
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^67^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=27477129), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=27477128) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=4157&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about the Melanocortin-1 receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CycMSH)]

Malignant melanoma is the deadliest form of skin cancer (1). Early and accurate diagnosis is necessary for surgery and successful treatment (2). The melanocortin (MC) system is a neuropeptide network of the skin, and it is involved in pigmentation regulation, cortisol production, and many other physiological processes (3). Most cutaneous cell types express MC receptors, proopiomelanocortin (POMC), and prohormone convertases, and they also release MCs. However, these receptors have been found to be overexpressed in melanoma cells. There are five MC receptors (MC1R to MC5R), which belong to the G-protein−coupled receptor superfamily. Melanotropin-stimulating hormones (α-, β-, and γ-MSH) are derived from POMC by the proteolytic action of prohormone convertases. α-MSH (Ac-Ser^1^-Tyr^2^-Ser^3^-Met^4^-Glu^5^-His^6^-Phe^7^-Arg^8^-Trp^9^-Gly^10^-Lys^11^-Pro^12^-Val^13^-NH_2_), produced by the brain and pituitary gland, is a tridecapeptide (13 amino acids) and is the most potent melanotropic peptide (4) in the regulation of skin pigmentation via MC1R.

Although positron emission tomography (PET) imaging with [^18^F]fluoro-2-deoxy-2-D-glucose ([^18^F]FDG) is effective in the detection of melanoma, it is not melanoma-specific and some melanoma cells do not take up [^18^F]FDG (5, 6). [^18^F]FDG has been approved (http://www.fda.gov/Drugs/DevelopmentApprovalProcess/Manufacturing/ucm182642.htm) for cancer imaging by the United States Food and Drug Administration. Radiolabeled α-MSH peptide analogs have been shown to specifically bind to MC1R that is overexpressed on human and mouse melanoma cells (5, 7-10). 1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) has been successfully coupled to the α-MSH peptide analogs for radiolabeling with a variety of radionuclides (5). A lactam bridge-cyclized α-MSH analog, GlyGlu-c[Lys-Nlc-Glu-His-D-Phe-Arg-Trp-Gly-Arg-Pro-Val-Asp] (GlyGlu-CycMSH), was conjugated with DOTA (11). DOTA-GlyGlu-CycMSH was radiolabeled with ^67^Ga as a potential molecular imaging agent to target melanoma (12). ^67^Ga is a positron emitter with a physical half-life of 3.3 d and is suitable for single-photon emission computed tomography (SPECT) imaging.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=MSH+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (MC1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=4157))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=155555)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CycMSH+and+synthesis)]

Guo et al. (12) reported the synthesis of ^67^Ga-DOTA-GlyGlu-CycMSH. The DOTA-GlyGlu-CycMSH peptide was synthesized using standard Fmoc chemistry on an amide resin with a peptide synthesizer. A solution of 10 µg DOTA-GlyGlu-CycMSH and 37 MBq (1 mCi) ^67^GaCl_3_ was incubated for 20 min at 90°C. ^67^Ga-DOTA-GlyGlu-CycMSH was purified with high-performance liquid chromatography (HPLC). Radiochemical purity (as confirmed with HPLC) was >95% with a labeling yield of >95%. The specific activity was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CycMSH+AND+in+vitro)]

Guo et al. (11) conducted in vitro competitive receptor-binding studies of DOTA-GlyGlu-CycMSH with B16/F1 murine melanoma cells that express the MC1R (~3,000 sites/cell). The radioactive ligand was ^125^I-Tyr^2^-[Nle^4^,D-Phe^7^]α-MSH. The inhibition concentration (IC_50_) was 2.4 nM.

Guo et al. (12) performed in vitro cellular internalization and efflux studies of ^67^Ga-DOTA-GlyGlu-CycMSH in B16/F1 melanoma cells. ^67^Ga-DOTA-GlyGlu-CycMSH exhibited 54% and 70% uptake of incubation dose inside the cells at 20 min and 90 min after incubation at 25°C, respectively. More than 80% of the internalized radioactivity remained inside the cells after 2 h of incubation in fresh medium.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CycMSH+AND+rodentia)]

Guo et al. (12) performed biodistribution studies in female C57BL/6 mice bearing 10-day-old B16/F1 murine melanoma tumors. Each mouse received an intravenous injection of 37 kBq (1 μCi) ^67^Ga-DOTA-GlyGlu-CycMSH. The radioactivity levels in percent injected dose per gram (% ID/g) were obtained at 0.5, 2, 4, and 24 h after injection (n = 5 mice per group). The tumor accumulation of ^67^Ga-DOTA-GlyGlu-CycMSH was 8.59 ± 1.37% ID/g at 0.5 h, 12.93 ± 1.63% ID/g at 2 h, 8.12 ± 0.60% ID/g at 4 h, and 5.02 ± 1.35% ID/g at 24 h, indicating high tumor retention. Coinjection of 10 μg DOTA-GlyGlu-CycMSH with ^67^Ga-DOTA-GlyGlu-CycMSH significantly reduced the tumor uptake to 0.37 ± 0.02% ID/g (P < 0.05) at 2 h after injection. No other organs showed a significant difference between the group that received DOTA-GlyGlu-CycMSH and the group that did not. With the exception of the kidneys, accumulation of ^67^Ga-DOTA-GlyGlu-CycMSH in nontarget tissues was low at 0.5 h, and the radioactivity was quickly cleared from most organs at 2 h after injection. Kidney accumulation was 24% ID/g at 0.5 h, 28% ID/g at 2 h, 23% ID/g at 4 h, and 21% ID/g at 24 h. The fast clearance from blood and normal organs (except the kidneys) and high tumor retention resulted in good tumor/nontarget organ ratios at 2 h (e.g., tumor/blood ratio of 259, tumor/muscle ratio of 323). When 15 mg L-lysine was coinjected with ^67^Ga-DOTA-GlyGlu-CycMSH, the kidney and tumor radioactivity levels were decreased by 70% and 0% at 2 h after injection, respectively.

SPECT/CT imaging of mice bearing the B16/F1 melanoma was conducted with injection of 7.1 MBq (0.2 mCi) ^67^Ga-DOTA-GlyGlu-CycMSH at 2 h. Only the tumor, kidneys, and urinary bladder were clearly visible. Coinjection of 30 μg DOTA-GlyGlu-CycMSH inhibited the tumor accumulation of radioactivity, whereas there was little effect on the kidney accumulation of radioactivity.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CycMSH+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CycMSH+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CycMSH+AND+human)]

No publication is currently available.

## NIH Support

P30 CA118100, P20 RR016480

## References

1 Jemal A., Siegel R., Ward E., Murray T., Xu J., Thun M.J. (2007). Cancer statistics, 2007. CA Cancer J Clin.
2 Miao Y., Hylarides M., Fisher D.R., Shelton T., Moore H., Wester D.W., Fritzberg A.R., Winkelmann C.T., Hoffman T., Quinn T.P. (2005). Melanoma therapy via peptide-targeted {alpha}-radiation. Clin Cancer Res.
3 Bohm M., Luger T.A., Tobin D.J., Garcia-Borron J.C. (2006). Melanocortin receptor ligands: new horizons for skin biology and clinical dermatology. J Invest Dermatol.
4 Catania A., Airaghi L., Garofalo L., Cutuli M., Lipton J.M. (1998). The neuropeptide alpha-MSH in HIV infection and other disorders in humans. Ann N Y Acad Sci.
5 Weiner R.E., Thakur M.L. (2005). Radiolabeled peptides in oncology: role in diagnosis and treatment. BioDrugs.
6 Dimitrakopoulou-Strauss A., Strauss L.G., Burger C. (2001). Quantitative PET studies in pretreated melanoma patients: a comparison of 6-[18F]fluoro-L-dopa with 18F-FDG and (15)O-water using compartment and noncompartment analysis. J Nucl Med.
7 Tatro J.B., Reichlin S. (1987). Specific receptors for alpha-melanocyte-stimulating hormone are widely distributed in tissues of rodents. Endocrinology.
8 Siegrist W., Solca F., Stutz S., Giuffre L., Carrel S., Girard J., Eberle A.N. (1989). Characterization of receptors for alpha-melanocyte-stimulating hormone on human melanoma cells. Cancer Res.
9 Miao Y., Whitener D., Feng W., Owen N.K., Chen J., Quinn T.P. (2003). Evaluation of the human melanoma targeting properties of radiolabeled alpha-melanocyte stimulating hormone peptide analogues. Bioconjug Chem.
10 Chen J., Cheng Z., Owen N.K., Hoffman T.J., Miao Y., Jurisson S.S., Quinn T.P. (2001). Evaluation of an (111)In-DOTA-rhenium cyclized alpha-MSH analog: a novel cyclic-peptide analog with improved tumor-targeting properties. J Nucl Med.
11 Guo H., Shenoy N., Gershman B.M., Yang J., Sklar L.A., Miao Y. (2009). Metastatic melanoma imaging with an (111)In-labeled lactam bridge-cyclized alpha-melanocyte-stimulating hormone peptide. Nucl Med Biol.
12 Guo H., Yang J., Shenoy N., Miao Y. (2009). Gallium-67-labeled lactam bridge-cyclized alpha-melanocyte stimulating hormone peptide for primary and metastatic melanoma imaging. Bioconjug Chem.